# 2-(5-[^18^F]Fluoro-pentyl)-2-methyl-malonic acid (ML-10)

Chemical name: | 2-(5-[^18^F]Fluoro-pentyl)-2-methyl-malonic acid (ML-10)
Abbreviated name: | [^18^F]ML-10
Synonym:
Agent Category: | Compound
Target: | Apoptotic cells
Target Category: | Other
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure of 2-(5-[^18^F]fluoro-pentyl)-2-methyl-malonic acid (ML-10) for more information in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=apoptosis&cmd=DetailsSearch)]

Radiotherapy, chemotherapy, or a combination of the two are often used in the clinic to induce apoptosis, the process of programed cell death, in cancerous tumor cells in order to treat neoplasms (1). Radiolabeled proteins, such as ^99m^Tc- or ^123^I-labeled annexin V and its derivatives that have a high affinity for externalized anionic phospholipids (e.g., phosphatidylserine (PS)) on apoptotic cells, were shown to be suitable for monitoring the efficacy and response to anticancer treatments with noninvasive imaging techniques such as single-photon emission tomography (2). In a preliminary study, it was shown that the ^99m^Tc-labeled C2A domain of synaptaganin I (binds to PS) can also be used for the imaging of non-small cell lung cancer tumor apoptosis in mice (3). However, none of these tracers can be used to visualize the progression of cell death in neoplastic lesions because these probes either have a slow clearance rate and generate a low signal/noise ratio, have unsuitable biodistribution characteristics, or tend to be immunogenic (4). Hence, there is much interest to develop and evaluate imaging probes that can be used with various imaging modalities, such as positron emission tomography (PET), to observe the initiation and progress of cellular apoptosis under normal and pathological conditions (4).

Damianovich et al. reported the development of a group of small molecule compounds, classified as ApoSense, and showed that systemic administration of a fluorescent or radiolabeled compound resulted in a selective accumulation of the tracer in apoptotic cells in three animal models of human cancers (5). A characteristic feature of the ApoSense compounds is that they are not transported across the cell membrane but pass through the plasma membrane and accumulate within the cytoplasm of apoptotic cells after initiation of apoptosis (6). To see a video of this phenomenon, click here (http://aposense.com/frontpage/Video.aspx). It was shown that two members of the ApoSense family, N,N'-didansyl-L-cystiene (DDC) (5) and 5-(dimethylamino)-1-napththalenesulfonyl-α-ethyl-[^18^F]fluoroalanine ([^18^F]NST-732) (6), can be used for the in vivo imaging of apoptosis in rodents with fluorescence (DDC and [^18^F]NST-732) and PET ([^18^F]NST-732) imaging techniques. In a continued effort to develop an ^18^F-labeled compound that can be used for the visualization of apoptosis with PET in the clinic, a small molecule with only a few functional moieties, 2-(5-[^18^F]fluoro-pentyl)-2-methyl-malonic acid ([^18^F]ML-10), was synthesized and evaluated for the detection of apoptotic cells in a mouse model of cerebral stroke (7). The biodistribution of [^18^F]ML-10 has been investigated in healthy rats (7) and healthy human volunteers (8). In another study, it was shown that [^18^F]ML-10 can be used with PET to detect the early response of metastases in the brain to whole-brain radiation therapy (9).

### Related Resource Links

Apoptosis related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=Apoptosis%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Apoptosis) (apoptosis)

Apoptosis pathways (http://pid.nci.nih.gov/search/intermediate_landing.shtml?molecule=Apoptosis&Submit=Go)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ML-10%20synthesis&cmd=DetailsSearch)]

The synthesis and purification of [^18^F]ML-10 with high-performance liquid chromatography (HPLC) has been described by Reshef et al. (7). The radiochemical yield (RCY) of HPLC-purified [^18^F]ML-10 was 30%–40% at the end of synthesis, with a radiochemical purity (RCP) of >99% and a specific activity (SA) of >40.7 GBq/μmol (1.505 Ci/μmol). The total time required for the synthesis was ~75 min.

An automated method for the synthesis of [^18^F]ML-10 has been described by Sobrio et al. (10). The RCY of the labeled compound was 39.8 ± 8.4% (n = 7 reactions), with an RCP of >99% and a SA of 235 ± 85 GBq/μmol (8.69 ± 3.14 Ci/μmol). The synthesis of [^18^F]ML-10 was completed in 70 min.

^3^H-Labeled ML-10 ([^3^H]ML-10) was synthesized for in vitro studies with Jurkat cells (a human T-cell leukemia cell line) as described elsewhere (7). Fluorescent dye-labeled dansyl-ML-10 was synthesized for the histopathological examination of tissues in some studies (8).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ML-10%20in%20vitro&cmd=DetailsSearch)]

The uptake of [^3^H]ML-10 was studied in Jurkat cells before apoptosis (control), after the induction of apoptosis (by exposure to anti-Fas antibody), and after the inhibition of apoptosis (by treatment with a caspase inhibitor) (7). Only cells undergoing apoptosis showed a significantly higher uptake (P < 0.001; ~9-fold) of radioactivity (1.87 ± 0.06% of total added radioactivity (% TAR)) compared with the control cells (0.20 ± 0.01% TAR) and the apoptosis-inhibited cells (0.25 ± 0.01% TAR).

In another study, the uptake of [^3^H]ML-10 by necrotic cells (Jurkat cells; necrosis induced by freeze-thaw cycles) was compared with that of control cells (7). A similar accumulation of radioactivity was observed both in the control cells and the necrotic cells.

Results obtained from these studies indicated that [^3^H]ML-10 accumulated selectively in the apoptotic cells and can distinguish the apoptotic cells from the normal and the necrotic cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ML-10%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^18^F]ML-10 was studied in healthy CD rats (http://www.criver.com/sitecollectiondocuments/cd-rat23.04.07.pdf) (7). The animals (n = 5 rats/time point) were given an intravenous injection (site not reported) of 0.37 MBq (~13.7 μCi) [^18^F]ML-10 and euthanized at time points ranging from 5 min postinjecton (p.i.) to 240 min p.i. The various organs of interest were harvested from the rats to determine the amount of radioactivity that accumulated in the tissues. Results were presented as percent of injected dose per gram tissue (% ID/g). No specific organ in the animals was observed to accumulate the tracer. All organs except the kidneys showed an uptake of <1% ID/g at 5 min p.i., and this level decreased gradually for up to 240 min p.i. At 5 min p.i., the kidneys showed an accumulation of 2.7 ± 0.88% ID/g of the tracer, and this level decreased to 0.05 ± 0.01% ID/g by 240 min p.i. The circulation half-life of the radiochemical was reported to be 23 min. The investigators concluded that the biodistribution of [^18^F]ML-10 in the rats was as expected because the labeled compound is not supposed to be taken up by healthy cells in tissues (7).

HPLC analysis of plasma and brain tissue obtained at 90 min p.i. from healthy rats injected with 50 MBq (1.85 mCi) [^18^F]ML-10 showed that >97% of the radiochemical was intact (7). This indicated that an insignificant amount of the labeled compound was metabolized in vivo.

Dynamic small-animal PET images were acquired from mice (number of animals not reported) with cerebral ischemia (induced by middle cerebral artery occlusion; MCAO mice) 45–90 min after injection of 0.37 MBq (~13.7 μCi) [^18^F]ML-10 (7). The images showed that the uptake of the tracer was multifocal, like a gradient, and was present only in the parenchyma of the cortical and subcortical regions of the affected left hemisphere of the brain. Very low levels of the tracer were evident in the unaffected contralateral cerebral hemisphere of the animals. Phosphorimaging and a histopathological examination of the brain sections obtained from MCAO mice injected with [^18^F]ML-10 showed that there was a correlation between areas showing the presence of radioactivity and the cells that exhibited the characteristics of apoptosis (r^2^ values not reported) (7).

In another study, male BALB/c mice (number not reported) were injected with 20 MBq (0.74 mCi) [^18^F]ML-10, and the anesthetized mice were subject to a whole-body PET scan for 120 min (8). From the images it was apparent that the tracer accumulated primarily in the testes of the animals. Histopathological examination of the testes obtained from mice treated with dansyl-ML-10 showed that the tracer accumulated only in those sections of the organs with apoptotic cells.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ML-10%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ML-10%20Non-Human%20Primates&cmd=DetailsSearch)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B18F%5DML-10%20Human%20Studies&cmd=DetailsSearch)]

The biodistribution of [^18^F]ML-10 was studied in 8 healthy human volunteers (four men and four women (mean age range, 21–44 y; weight, 69 ± 11 kg)) (8). The individuals were given an intravenous injection of 233 ± 90 MBq (8.6 ± 3.3 mCi) [^18^F]ML-10, and whole-body PET/computed tomography (CT) scans were acquired from the subjects for up to 220 min p.i. as detailed by Hoglund et al. (8). The images showed that the tracer was cleared from all the non-target organs and excreted into the urinary bladder by 10 min p.i. The blood circulation half-life and the organ elimination half-life of the tracer were 1.3 ± 0.1 h and 1.1 ± 0.2 h, respectively. All male subjects showed an accumulation of the probe in the testes as reported with the male mice (see above). The accumulation of tracer in the testes peaked at ~25 min p.i., plateaued at ~90 min p.i., and showed a gradual decrease after this time point. The biodistribution profile of [^18^F]ML-10 was observed to be similar among all the male and female subjects enrolled in the study. From this study, the investigators concluded that, because [^18^F]ML-10 had a suitable biodistribution and safety profile in humans, it can be developed as a PET agent for the detection of apoptosis in the clinic (8).

The use of [^18^F]ML-10 was evaluated in 10 patients to assess the response of brain metastases to whole-brain radiation therapy (9). Each patient underwent a baseline PET scan (before initiation of radiation treatment) and a PET scan after radiotherapy (after 9 or 10 treatments). The amount of [^18^F]ML-10 administered to each participant did not exceed ~0.5 GBq (13.5 mCi). Magnetic resonance images (MRI) were acquired from each patient at 6–8 weeks after completion of the radiation treatment. In all patients, the brain lesions were detectable with both [^18^F]ML-10 PET and MRI scans. In addition, a high correlation was observed between the early changes noticed with PET scans and the alteration in tumor anatomical dimensions observed later with the MRI scans (r = 0.9). Only 9 patients completed the pre- and post-treatment [^18^F]ML-10 PET/CT scans (9). From the post-treatment scan images, the ratios of mean uptake of radioactivity in the lesion (signal) and the corresponding contralateral healthy brain tissues (background) were determined. The mean signal/background ratios for scans performed at 20–36 min p.i., 80–100 min p.i., and 130–150 min p.i. were 4.62 ± 2.64, 6.63 ± 3.81, and 8.76 ± 5.59, respectively. This indicated that the tracer accumulated in the cancerous lesions over time but was cleared rapidly from the noncancerous areas of the brain. From this study, the investigators concluded that [^18^F]ML-10 was probably suitable to determine tumor responsiveness to anticancer therapy in humans (9).

In another study [^18^F]ML-10 was used for the imaging of apoptotic neurovascular cells in patients with acute ischemic cerebral stroke (11).

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Haimovitz-Friedman A., Yang T.I., Thin T.H., Verheij M. (2012). Imaging radiotherapy-induced apoptosis. Radiat Res.
2 De Saint-Hubert M., Bauwens M., Verbruggen A., Mottaghy F.M. (2012). Apoptosis imaging to monitor cancer therapy: the road to fast treatment evaluation?. Curr Pharm Biotechnol.
3 Wang F., Fang W., Zhao M., Wang Z., Ji S., Li Y., Zheng Y. (2008). Imaging paclitaxel (chemotherapy)-induced tumor apoptosis with 99mTc C2A, a domain of synaptotagmin I: a preliminary study. Nucl Med Biol.
4 Cohen A., Shirvan A., Levin G., Grimberg H., Reshef A., Ziv I. (2009). From the Gla domain to a novel small-molecule detector of apoptosis. Cell Res.
5 Damianovich M., Ziv I., Heyman S.N., Rosen S., Shina A., Kidron D., Aloya T., Grimberg H., Levin G., Reshef A., Bentolila A., Cohen A., Shirvan A. (2006). ApoSense: a novel technology for functional molecular imaging of cell death in models of acute renal tubular necrosis. Eur J Nucl Med Mol Imaging.
6 Aloya R., Shirvan A., Grimberg H., Reshef A., Levin G., Kidron D., Cohen A., Ziv I. (2006). Molecular imaging of cell death in vivo by a novel small molecule probe. Apoptosis.
7 Reshef A., Shirvan A., Waterhouse R.N., Grimberg H., Levin G., Cohen A., Ulysse L.G., Friedman G., Antoni G., Ziv I. (2008). Molecular imaging of neurovascular cell death in experimental cerebral stroke by PET. J Nucl Med.
8 Hoglund J., Shirvan A., Antoni G., Gustavsson S.A., Langstrom B., Ringheim A., Sorensen J., Ben-Ami M., Ziv I. (2011). 18F-ML-10, a PET tracer for apoptosis: first human study. J Nucl Med.
9 Allen A.M., Ben-Ami M., Reshef A., Steinmetz A., Kundel Y., Inbar E., Djaldetti R., Davidson T., Fenig E., Ziv I. (2012). Assessment of response of brain metastases to radiotherapy by PET imaging of apoptosis with (18)F-ML-10. Eur J Nucl Med Mol Imaging.
10 Sobrio, F., M. Medoc, L. Martial, J. Delamare, and L. Barre, Automated Radiosynthesis of [(18)F]ML-10, a PET Radiotracer Dedicated to Apoptosis Imaging, on a TRACERLab FX-FN Module. Mol Imaging Biol, 2012
11 Reshef A., Shirvan A., Akselrod-Ballin A., Wall A., Ziv I. (2010). Small-molecule biomarkers for clinical PET imaging of apoptosis. J Nucl Med.